# N-(6-[^18^F]Fluoro-4-phenoxypyridin-3-yl)-N-(2-methoxybenzyl)acetamide

Chemical name: | N-(6-[^18^F]Fluoro-4-phenoxypyridin-3-yl)-N-(2-methoxybenzyl)acetamide
Abbreviated name: | 6-[^18^F]Fluoro-PBR28
Synonym: | [^18^F]15
Agent Category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR; 18-kDa translocator protein (TSPO))
Target Category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal / contrast: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on above structure of 6-[^18^F]fluoro-PBR28 for more information in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=translocator%20protein%2018%20kda&cmd=DetailsSearch)]

The 18-kDa translocator protein (TSPO; also known as the peripheral benzodiazepine receptor (PBR)) is evolutionarily conserved and is found mainly in the outer membrane of the mitochondria of steroid-synthesizing tissues, including the brain (1). Although the TSPO is involved in neuroinflammation and axonal regeneration after brain injury (2), the best characterized function of this protein is the transport of cholesterol from the outer membrane of the mitochondria to the inner membrane of these organelles, where it is used for steroid and neurosteroid hormone synthesis (2). Very low levels of TSPO are expressed in healthy brain tissue, but, in the event of an injury, the protein is overexpressed at the site of injury (3) both in the peripheral nervous system (in Schwann cells, macrophages, and neurons) and in the central nervous system (in activated microglia and infiltrating macrophages) (1). In addition, TSPO is overexpressed in different types of neuroinflammatory diseases such as Alzheimer’s disease, Parkinson’s disease, stroke, and various cancers, including those of the brain (3), but the expression of this protein is downregulated in psychiatric disorders such as anxiety, schizophrenia, depression, and bipolar disorder (1). Because the TSPO density is altered during neuronal injury or disease, it has been suggested that TSPO may serve as a biomarker of neuroinflammation and may be used to determine the efficacy of drugs used to monitor the progression and treatment of neuroinflammatory diseases (3). Several TSPO-selective ligands with diverse chemical structures have been synthesized, radiolabeled with ^11^C or ^18^F, and evaluated with positron emission tomography (PET) for the noninvasive imaging of this receptor in the brain of various species of animals (mouse, rat, and monkey) (4). For a detailed discussion of the chemistry of different TSPO ligands, see Dolle et al. (3). It is not clear, however, how the labeled ligands interact with the TSPO, and much is unknown about the changes that take place within this protein during neuroinflammation and related disorders (5).

[^11^C]PK11195 targets TSPO and is commonly used with PET for the imaging of neurological disorders, but its uptake in the brain can be difficult to quantify because the tracer has high lipophilicity and exhibits high nonspecific binding (6). Much effort has been devoted to develop and screen new tracers that can be used for the imaging and quantification of TSPO (such as [^11^C]DAA1106, [^18^F]DAA1106, [^18^F]FEDAA1106, [^11^C]PBR28, etc.) (4, 6). However, these radioligands have to be synthesized with multi-step procedures, and all of them are still under investigation for use in animals (4). Using a single-step procedure, Damont et al. synthesized N-(6-[^18^F]fluoro-4-phenoxypyridin-3-yl)-N-(2-methoxybenzyl)acetamide (6-[^18^F]Fluoro-PBR28), a radiofluorinated derivative of PBR28, studied its characteristics in vitro, and evaluated the tracer for the imaging of TSPO in the rat brain (4).

### Related Resource Links

Related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D)

Human TSPO in Gene Database (http://www.ncbi.nlm.nih.gov/gene?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D). Gene ID: 706

TSPO in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/109610))

Clinical trials (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR) related to PET imaging of TSPO

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-%5B18F%5DFluoro-PBR28%20synthesis&cmd=DetailsSearch)]

The synthesis and ^18^F-labeling of 6-Fluoro-PBR28 has been detailed by Damont et al. (4). The radiochemical yield of the labeled compound was 16%–18% (n > 10 reactions), with a radiochemical purity of >99%. The specific activity of 6-[^18^F]Fluoro-PBR28 was reported to be 74–148 GBq/μmol (2–4 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-%5B18F%5DFluoro-PBR28%20in%20vitro%20studies&cmd=DetailsSearch)]

The log D_7.4_ (n-octanol/buffer pH 7.4 partition coefficient) and log P (n-octanol/water partition coefficient) of 6-[^18^F]Fluoro-PBR28 were determined to be 2.82 ± 0.14 and 2.77 ± 0.10, respectively (4).

Using [^3^H]PK11195 as the ligand in a competition assay, the binding affinities (K_i_) of 6-Fluoro-PBR28 for TSPO in rat heart homogenate, rat kidney mitochondrial-enriched fraction, and the mitochondrial fraction of HEK293 cells (originating from human embryonic kidney) were reported to be 0.44 ± 0.01 nM, 3.90 ± 0.30 nM, and 1.19 ± 0.03 nM, respectively (4). The K_i_ values of PK11195 in these preparations were determined to be 1.80 ± 0.04 nM, 9.30 ± 0.50, and 7.11 ± 0.35, respectively. This indicated that 6-Fluoro-PBR28 had a higher binding affinity for TSPO compared with PK11195.

In another study with rat glioma C6 cells, 6-Fluoro-PBR28 was observed to have a lower stimulation of pregnenolone (a precursor of steroid hormones) synthesis (16.46 ± 1.77% above controls) compared with PK11195 (37.0 ± 1.0% above control) (4). This indicated that the PBR28 derivative had a lower potency than PK11195 to stimulate steroidogenesis in the rat cells.

Ex vivo binding studies were performed with brain sections obtained from rats treated with α-amino-3-hydroxy-5-methylisoxazol-4-propionate (AMPA; 7.5 nmol) to induce inflammatory lesions in the organ (4). Autoradiography of brain sections exposed to 6-[^18^F]Fluoro-PBR28 in presence or absence of nonradioactive 6-Fluoro-PBR28 or PK11195 (20 nM) showed that only those sections that were exposed to 6-[^18^F]Fluoro-PBR28 alone had a high ipsi/contralateral ratio (value not reported). This indicated that the ^18^F-labeled derivative of PRB28 had a high specificity of binding to TSPO.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-%5B18F%5DFluoro-PBR28%20rodentia&cmd=DetailsSearch)]

Acute neuroinflammatory lesions were induced with a stereotaxic injection of 7.5 nmol AMPA in rats for micro-PET imaging with 6-[^18^F]Fluoro-PBR28 and [^11^C]PK11195, respectively (4). The animals (number not reported) were injected with one of the two labeled compounds (concentration of tracer and route of injection were not reported), and micro-PET images of the brain were acquired for up to 60 min postinjection (p.i.). At 60 min p.i., the AMPA-induced lesions were clearly visible in the axial, coronal, and sagittal PET images of the animals (results for [^11^C]PK11195 were not reported). Time-activity curves of 6-[^18^F]Fluoro-PBR28 showed that maximum uptake of radioactivity (~0.5% injected dose per cubic centimeter of tissue (% ID/cc)) from the tracer was reached within 1–2 min p.i. and remained constant for the duration of the study (60 min p.i.), and the ipsi/contralateral uptake ratio at the 1-2 min time point was 2.2. Uptake kinetics observed with [^11^C]PK11195 within the first 1–2 min p.i. (maximum uptake, ~0.4% ID/cc) were similar to uptake kinetics observed with [^18^F]Fluoro-PBR28, but a rapid clearance of label from the lesions was observed with the ^11^C-labeled compound; by 60 min p.i., the amount of radioactivity in the lesions decreased to ~0.25% ID/cc.

From these preliminary studies, the investigators concluded that 6-[^18^F]Fluoro-PBR28 was probably suitable for the PET imaging of neuroinflammatory lesions in the brain of rodents (4).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-%5B18F%5DFluoro-PBR28%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No reference is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=21741237%5Buid%5D&cmd=DetailsSearch)]

No reference is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=6-%5B18F%5DFluoro-PBR28%20Human%20Studies&cmd=DetailsSearch)]

No reference is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Rupprecht R., Papadopoulos V., Rammes G., Baghai T.C., Fan J., Akula N., Groyer G., Adams D., Schumacher M. (2010). Translocator protein (18 kDa) (TSPO) as a therapeutic target for neurological and psychiatric disorders. Nat Rev Drug Discov.
2 Girard C., Liu S., Adams D., Lacroix C., Sineus M., Boucher C., Papadopoulos V., Rupprecht R., Schumacher M., Groyer G. (2012). Axonal regeneration and neuroinflammation: roles for the translocator protein 18 kDa. J Neuroendocrinol.
3 Dolle F., Luus C., Reynolds A., Kassiou M. (2009). Radiolabelled molecules for imaging the translocator protein (18 kDa) using positron emission tomography. Curr Med Chem.
4 Damont A., Boisgard R., Kuhnast B., Lemee F., Raggiri G., Scarf A.M., Da Pozzo E., Selleri S., Martini C., Tavitian B., Kassiou M., Dolle F. (2011). Synthesis of 6-[(1)(8)F]fluoro-PBR28, a novel radiotracer for imaging the TSPO 18 kDa with PET. Bioorg Med Chem Lett.
5 Scarf A.M., Kassiou M. (2011). The translocator protein. J Nucl Med.
6 Doorduin J., de Vries E.F., Dierckx R.A., Klein H.C. (2008). PET imaging of the peripheral benzodiazepine receptor: monitoring disease progression and therapy response in neurodegenerative disorders. Curr Pharm Des.